# Microbubbles conjugated with knottin 2.5D

Chemical name: | Microbubbles conjugated with knottin 2.5D
Abbreviated name: | MB_Knottin_
Synonym:
Agent Category: | Peptide
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptor
Method of detection: | Ultrasound
Source of signal / contrast: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Ultrasound is the most widely used imaging modality in clinical medicine (1) and its role in noninvasive molecular imaging with ligand-carrying microbubbles is expanding (2). Microbubbles are comprised of spherical cavities filled by a gas encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin, or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of microbubbles. Microbubbles are usually 1–8 μm in diameter. They provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They are also potentially used for drug and gene delivery (6).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (12, 14, 15). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (e.g., vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (16).

Microbubbles conjugated to either peptides or antibodies against integrins, cell adhesion molecules, and VEGF receptors have previously been studied for the noninvasive assessment and imaging of tumor angiogenesis (17-20). Cystine knot peptides (knottins) share a common disulfide-bonded framework and a triple-stranded β-sheet fold (21). The integrin-binding RGD motif was grafted into a knottin from trypsin inhibitor II of the squash plant (Ecballium elaterium). Knottin 2.5D (with three disulfide bonds; GCPQGRGDWAPTSCSQDSDCLAGCVCGPNGFCG-NH_2_) was identified from a series of genetically engineered knottin peptides to have nanomolar binding to the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors (22, 23). Willmann et al. (24) studied ultrasonic imaging of tumor vasculature using microbubbles conjugated with knottin 2.5D (MB_Knottin_) in mice bearing human tumor xenografts.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Knottin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Knottin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=841163))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=knot%20peptide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubble+knottin+synthesis)]

Knottin 2.5D was prepared with solid-phase peptide synthesis (24). The linear peptide was folded in the presence of 2.5 mM reduced glutathione and 20% dimethylsulfoxide in 0.1 M ammonium bicarbonate (pH, 9). Both peptides were purified with high-performance liquid chromatography. Peptide purity and molecular mass were confirmed with MALDI-TOF mass spectroscopy and electrospray ionization mass spectrometery. Knottin was biotinylated at its N-terminus for conjugation with perfluorocarbon-filled microbubbles (1.5 ± 0.1 µm) through biotin-streptavidin interaction to yield MB_Knottin_. Three other microbubbles were also prepared: microbubbles coupled to a biotinylated scrambled knottin peptide (MB_scrambled_), microbubbles coupled to a biotinylated rat anti-mouse α_v_β_3_ integrin (MB_αvβ3_), and microbubbles coupled to a biotinylated c(RGDfK) (MB_cRGD_). The number of ligands per µm^2^ of microbubble surface was estimated to be ~7,600.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubble+knottin+in+vitro+studies)]

Willmann et al. (24) reported that MB_Knottin_, MB_scrambled_, MB_αvβ3_, or MB_cRGD_ (7 × 10^6^/ml) perfused through the flow chamber coated with integrin-positive mouse angiosarcoma endothelial cells at a wall shear rate of 100 s^-1^ for ~3 min. There was a significantly (P < 0.001) greater number of MB_Knottin_ attached to the endothelial cells (1.76 ± 0.49 MBs/cell) than the other three microbubble preparations (MB_scrambled_, 0.15 ± 0.12; MB_αvβ3_, 0.60 ± 0.07; MB_cRGD_, 0.74 ± 0.32). Pretreatment with excess c(RGDyK) reduced the binding of MB_Knottin_ to 0.20 ± 0.16 MBs/cell (P < 0.04). All four microbubble preparations showed minimal binding (<0.13 MBs/cells) to integrin-negative mouse breast cancer cells (4T1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubble+knottin+rodentia)]

Willmann et al. (24) performed ultrasound assessment of microbubble binding in 9–19 mice bearing human ovarian adenocarcinoma SKOV-3 tumors at 4 min after injection of MB_Knottin_, MB_scrambled_, MB_αvβ3_, or MB_cRGD_ (7 × 10^6^). The tumor video intensities were 11.9 ± 6.1, 5.2 ± 1.0, 5.6 ± 2.3, and 7.1 ± 7.9 for MB_Knottin_, MB_scrambled_, MB_αvβ3_, and MB_cRGD_, respectively. The binding of MB_Knottin_ to the tumors was significantly higher than that of the other microbubbles tested (P < 0.05). Pretreatment with excess c(RGDyK) (30 min before MB_Knottin_) reduced the tumor video intensity to 4.7 ± 4.0 (P < 0.05). The muscle video intensity was 1.3 ± 0.3 for MB_Knottin_. Immunofluorescence staining of frozen SKOV-3 tumor sections showed the localization of β_3_ integrin to the tumor endothelial cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubble+knottin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubble+knottin+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubble+knottin+Human+Studies)]

No references are currently available.

## NIH Support

5K01 CA104706, R21 CA139279, P50 CA114747

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
15 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
16 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
17 Villanueva F.S., Jankowski R.J., Klibanov S., Pina M.L., Alber S.M., Watkins S.C., Brandenburger G.H., Wagner W.R. (1998). Microbubbles targeted to intercellular adhesion molecule-1 bind to activated coronary artery endothelial cells. Circulation.
18 Weller G.E., Lu E., Csikari M.M., Klibanov A.L., Fischer D., Wagner W.R., Villanueva F.S. (2003). Ultrasound imaging of acute cardiac transplant rejection with microbubbles targeted to intercellular adhesion molecule-1. Circulation.
19 Weller G.E., Villanueva F.S., Klibanov A.L., Wagner W.R. (2002). Modulating targeted adhesion of an ultrasound contrast agent to dysfunctional endothelium. Ann Biomed Eng.
20 Reinhardt M., Hauff P., Linker R.A., Briel A., Gold R., Rieckmann P., Becker G., Toyka K.V., Maurer M., Schirner M. (2005). Ultrasound derived imaging and quantification of cell adhesion molecules in experimental autoimmune encephalomyelitis (EAE) by Sensitive Particle Acoustic Quantification (SPAQ). Neuroimage.
21 Pallaghy P.K., Nielsen K.J., Craik D.J., Norton R.S. (1994). A common structural motif incorporating a cystine knot and a triple-stranded beta-sheet in toxic and inhibitory polypeptides. Protein Sci.
22 Kimura R.H., Levin A.M., Cochran F.V., Cochran J.R. (2009). Engineered cystine knot peptides that bind alphavbeta3, alphavbeta5, and alpha5beta1 integrins with low-nanomolar affinity. Proteins.
23 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
24 Willmann J.K., Kimura R.H., Deshpande N., Lutz A.M., Cochran J.R., Gambhir S.S. (2010). Targeted contrast-enhanced ultrasound imaging of tumor angiogenesis with contrast microbubbles conjugated to integrin-binding knottin peptides. J Nucl Med.